# 4-[^18^F]Fluoropaclitaxel

Chemical name: | 4-[^18^F]Fluoropaclitaxel
Abbreviated name: | [^18^F]FPAC
Synonym: | [^18^F]Taxol®
Agent category: | Compound
Target: | P-glycoprotein (P-gp) multidrug transporter, MDR-1
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20paclitaxel%20or%20fluoropaclitaxel%29)]

One of the mechanisms that tumor cells use to escape the cytotoxic effects of chemotherapeutic agents, such as Adriamycin, Vinca alkaloids, epipodophyllotoxins, actinomycin D, and paclitaxel (PAC), is to limit their presence inside the cells through the actions of P-glycoprotein (P-gp), a protein encoded by the multidrug resistance (MDR-1) gene (1, 2). P-gp is an ATP-dependent transmembrane multidrug transporter that is capable of actively pumping a variety of agents out of cells. Injection of unlabeled efflux pump substrates increases the retention of radioactivity in tumors rather than lessening the retention, as seen with receptor-binding radiotracers. Overexpression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood-brain barrier (4, 5). Calcium channel blockers, cyclosporin A, and its non-immunosuppressive analog PSC 833 are MDR modulators that inhibit transport of P-gp substrates out of cells (6, 7).

Sestamibi (MIBI) is a substrate for P-gp. ^99m^Tc-MIBI has been approved by the United States Food and Drug Administration (FDA) as a myocardial perfusion imaging agent for use with single-photon emission computed tomography (SPECT) to assess the risk of future cardiac events. It is also approved as a tumor-imaging agent in breast, lung, thyroid, and brain cancers. PAC is an FDA-approved chemotherapeutic agent exerting its antitumor activity by binding to β-tubulin to inhibit cell division (8). It is also a transport substrate for P-gp in tumor cells, leading to drug-related resistance to chemotherapy (8, 9). Therefore, [^18^F]fluoropaclitaxel ([^18^F]FPAC) is being developed as a positron emission tomography (PET) agent to noninvasively study P-gp function and multidrug resistance in tumors and normal tissues.

### Related Resource Links:

- Chapters in MICAD (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (P-glycoprotein (http://www.ncbi.nlm.nih.gov/gene/5243))
- Articles in OMIM (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D))
- Clinical trials (P-glycoprotein (http://www.clinicaltrials.gov/ct2/results?term=P-glycoprotein), ^99m^Tc-MIBI (http://www.clinicaltrials.gov/ct2/results?term=Sestamibi), Paclitaxel (http://www.clinicaltrials.gov/ct2/results?term=paclitaxel))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc-sestamibi+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=16), Paclitaxel (http://google2.fda.gov/search?q=paclitaxel&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20paclitaxel%20or%20fluoropaclitaxel%29%20and%20synthesis)]

Kiesewetter et al. (10) prepared [^18^F]FPAC by incorporating [^18^F]fluoride (Kryptofix 2.2.2 and K_2_CO_3_) into [^18^F]fluorobenzoate ester via nucleophilic displacement of a trimethylammonium moiety. The ester group was removed, and the resulting [^18^F]fluorobenzoic acid was coupled to 3´-debenzoylpaclitaxel (10).The final product was purified by high-performance liquid chromatography. The radiochemical yield for the syntheses was 18.3 ± 5.5% (not corrected for decay). The specific activity at the end of bombardment was 169-453 GBq/mmol (4.58-12.25 Ci/mmol) for 14 syntheses. The total synthesis time was 80 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20fluoropaclitaxel%20%29%20and%20in%20vitro)]

In an in vitro study using human hepatocytes, 50% [^18^F]FPAC was metabolized to produce one major metabolite, 6α-hydroxy-FPAC, after 4 h of incubation (10). In rat hepatocytes, 3 metabolites were produced from [^18^F]FPAC with a half-life of 194 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20paclitaxel%20or%20fluoropaclitaxel%29%20and%20rodentia)]

Biodistribution studies in normal rats showed high accumulation of radioactivity, as measured by differential uptake ratio, in the liver (1.64), followed by the kidney (1.59), heart (1.28), and lung (0.99) at 60 min after injection of [^18^F]FPAC (10). Levels of the tracer were low in the brain (0.018) and blood (0.08). Pretreatment (20 min) with PAC (200 nmol) increased [^18^F]FPAC accumulation in the blood (33%), heart (32%), lung (38%), liver (30%), kidney (142%), and brain (5%). Increased accumulation is consistent with saturation of the efflux pump, P-gp. There was a significantly greater accumulation of [^18^F]FPAC in the heart (79% increase), lung (143%), muscle (38%), and brain (1300%) in mdr1a/1b(-/-) mice than in wild-type mice. Furthermore, biodistribution studies in both types of mice with pre-injection of PAC or XR9576, an MDR modulator, showed little effect on the accumulation of [^18^F]FPAC in the knockout mice compared with the wild-type mice, which showed significant increases only in the lung and kidney. The kidney contained 42-71% intact [^18^F]FPAC, whereas the liver contained 59-86% at 30 min after injection in both types of mice.

Biodistributions of [^18^F]FPAC and [^3^H]PAC were very similar in nude mice bearing MCF-7 human breast tumors, with the highest accumulations in the small intestine, the lowest accumulations in the brain, and intermediate accumulations in the tumor (11). Uptake in these and other tissues was not significantly inhibited or enhanced by the presence of unlabeled PAC (20 mg/kg). Administration of cyclosporin A (10 mg/kg) increased uptake of both [^18^F]FPAC and [^3^H]PAC into the tumor by 1-fold.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20fluoropaclitaxel%29%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F-paclitaxel%20or%20fluoropaclitaxel%29%20and%20%28nonhuman%20primate%29)]

Kurdziel et al. (12) performed PET imaging in 3 rhesus monkeys after injection of 222-444 MBq (6-12 mCi) of [^18^F]FPAC. Pretreatment with XR9576 (a P-gp blocker) changed the Logan plot slope (distribution volume) for the liver by +104% (P = 0.02), the lung by +87% (P = 0.01), and the kidney by -14% (P = 0.08) (12). Changes in the mean area under time-activity curve (AUC; plasma metabolite-corrected) were +54% (P = 0.08), +97% (P = 0.04), and -12% (P = 0.02), respectively, for the liver, lung, and kidney. This indicates that accumulation of [^18^F]FPAC in the liver and lung is modulated by the MDR P-gp efflux pump. No significant difference was found in the AUC between the baseline and XR9576 studies.

Kurdziel et al. (12) estimated the human dosimetry of [^18^F]FPAC in 3 rhesus monkeys after injection of 222-444 MBq (6-12 mCi) of [^18^F]FPAC. The organs that received the highest absorbed doses were the gallbladder (0.19 mGy/MBq, or 0.69 rad/mCi), the liver (0.14 mGy/MBq, or 0.52 rad/mCi), upper intestine (0.094 mGy/MBq, or 35 rad/mCi), and the kidneys (0.044 mGy/MBq, or 0.163 rad/mCi). The effective dose was 0.022 mSv/MBq (0.083 rem/mCi).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F-paclitaxel%20or%20fluoropaclitaxel%29%20and%20%28%20human%29)]

Kurdziel et al. (13) estimated the human dosimetry of [^18^F]FPAC in 3 healthy subjects after injection of 192.4 MBq (5.2 mCi) of [^18^F]FPAC. The organs receiving the highest radiation dose were the gallbladder, large intestine and small intestine at 0.23 mGy/MBq (0.85 rad/mCi), 0.19 mGy/MBq (0.68 rad/mCi), and 0.16 mGy/MBq (0.60 rad/mCi), respectively. The effective dose was 28.79 μSv/MBq (0.107 rem/mCi). [^18^F]FPAC PET studies were performed with dynamic scans for 60 min and static scans for 120 min in 3 breast cancer patients. The tumor uptake was low with an average maximum standard uptake value (SUV_max_) of 1.8 at 80 s after injection decreased slightly over time. When compared with background tissue (contralateral breast), the tumors were visible with an average maximum tumor/background ratio of 7.7 at 20 min. Tumor/blood ratios increased slightly over time to an average maximum of 1.9.

## NIH Support

Intramural Research Program, 1R21 CA098334-01A1

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Thiebaut F., Tsuruo T., Hamada H., Gottesman M.M., Pastan I., Willingham M.C. (1987). Cellular localization of the multidrug-resistance gene product P-glycoprotein in normal human tissues. Proc Natl Acad Sci U S A.
6 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
7 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
8 Horwitz S.B., Cohen D., Rao S., Ringel I., Shen H.J., Yang C.P. (1993). Taxol: mechanisms of action and resistance. J Natl Cancer Inst Monogr.
9 Huang Y., Ibrado A.M., Reed J.C., Bullock G., Ray S., Tang C., Bhalla K. (1997). Co-expression of several molecular mechanisms of multidrug resistance and their significance for paclitaxel cytotoxicity in human AML HL-60 cells. Leukemia.
10 Kiesewetter D.O., Jagoda E.M., Kao C.H., Ma Y., Ravasi L., Shimoji K., Szajek L.P., Eckelman W.C. (2003). Fluoro-, bromo-, and iodopaclitaxel derivatives: synthesis and biological evaluation. Nucl Med Biol.
11 Gangloff A., Hsueh W.A., Kesner A.L., Kiesewetter D.O., Pio B.S., Pegram M.D., Beryt M., Townsend A., Czernin J., Phelps M.E., Silverman D.H. (2005). Estimation of paclitaxel biodistribution and uptake in human-derived xenografts in vivo with (18)F-fluoropaclitaxel. J Nucl Med.
12 Kurdziel K.A., Kiesewetter D.O., Carson R.E., Eckelman W.C., Herscovitch P. (2003). Biodistribution, radiation dose estimates, and in vivo Pgp modulation studies of 18F-paclitaxel in nonhuman primates. J Nucl Med.
13 Kurdziel K.A., Kalen J.D., Hirsch J.I., Wilson J.D., Bear H.D., Logan J., McCumisky J., Moorman-Sykes K., Adler S., Choyke P.L. (2011). Human dosimetry and preliminary tumor distribution of 18F-fluoropaclitaxel in healthy volunteers and newly diagnosed breast cancer patients using PET/CT. J Nucl Med.